# Gadolinium-bis-5-hydroxytriptamide-diethylenetriamine pentaacetic acid

Chemical name: | Gadolinium-bis-5-hydroxytriptamide-diethylenetriamine pentaacetic acid
Abbreviated name: | Gd-bis-5-HT-DTPA
Synonym: | MPO-Gd
Agent Category: | Compound
Target: | Myeloperoxidase (MPO)
Target Category: | Enzyme
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Gd
Activation: | Yes
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MPO-Gd&cmd=DetailsSearch)]

Inflammation is believed to be a precursor to a variety disorders such as diabetes (http://www.ncbi.nlm.nih.gov/pubmedhealth/PMH0002194/), cardiovascular diseases (http://www.webmd.com/heart-disease/guide/diseases-cardiovascular), chronic obstructive pulmonary disease (http://www.ncbi.nlm.nih.gov/pubmedhealth/PMH0001153/), depression (http://www.ncbi.nlm.nih.gov/pubmedhealth/PMH0003697/), dementia (http://www.ncbi.nlm.nih.gov/pubmedhealth/PMH0001748/), cancers (http://www.ncbi.nlm.nih.gov/pubmedhealth/PMH0002267/), etc., and low-grade systemic inflammation is recognized as a predictor of the development of most of these diseases (1). The process of inflammation is triggered when there is an anticipated or real threat (infection, injury, etc.) to tissue homeostasis, and the main aim of this response is to diminish the threat and begin repairs at the site of distress (2). Once the process of inflammation is initiated, there is a recruitment of myeloid cells (neutrophils, microglia, and macrophages) at the site of the trauma, and these cells secrete a variety of pro-inflammation mediators, including myeloperoxidase (http://www.uniprot.org/uniprot/P05164) (MPO), a heme-containing enzyme that helps maintain the inflammatory state of the tissue. MPO is produced and secreted mainly by the myeloid cells, metabolizes hydrogen peroxide (H_2_O_2_) to produce elevated levels of cytotoxic reactive oxygen species (e.g., hypochlorous acid, HOCl), and promotes further tissue injury and inflammation at the site of recruitment (3, 4). Therefore, the quantification of MPO activity in normal and inflamed tissue could be an excellent biomarker to predict the potential development and progression of the various inflammatory disorders (5). For this, investigators developed gadolinium-bis-5-hydroxytriptamide-diethylenetriamine pentaacetic acid (Gd-bis-5-HT-DTPA; also known as MPO-Gd), a magnetic resonance imaging (MRI) agent, that acts as a substrate for the MPO and used it for the noninvasive visualization of MPO activity in normal and diseased tissues (3).

Oxidative activation of the paramagnetic substrate (Gd-bis-5-HT-DTPA) by MPO leads to oligomerization and entrapment of the activated Gd-bis-5-HT-DTPA within the tissue by cross-linking the monomer or the oligomer with tyrosine-containing proteins, thereby increasing the localized concentration Gd at the site of MPO activity as explained in detail by Rodriguez et al. (5). In addition, the oligomeric and entrapped Gd-bis-5-HT-DTPA has a slow clearance rate from the tissue compared to the non-activated compound, and delayed clearance of the activated Gd-bis-5-HT-DTPA allows for the imaging of MPO in the inflamed tissue.

### Related Resource Links

Human myeloperoxidase nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_009629.1) and protein (http://www.ncbi.nlm.nih.gov/protein/NP_000241.1) sequences

Clinical trials (http://clinicaltrials.gov/ct2/results?term=myeloperoxidase) related to myeloperoxidase

Myeloperoxidase related pathways in Pathways Interaction Database (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=myeloperoxidase&Submit=Go)

Myeloperoxidase in Online Mendelian Inheritance in Man Database (OMIM) (http://omim.org/entry/606989)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gd-bis-5-HT-DTPA%20synthesis&cmd=DetailsSearch)]

The synthesis of Gd-bis-5-HT-DTPA has been described by Rodriguez et al. (5). The final product (yield not reported) was purified with high-performance liquid chromatography and had a purity of >96%. The molecular weight of purified Gd-bis-5-HT-DTPA was determined to be 707.33 (expected 707.22) with mass spectroscopy analysis.

The biodistribution of Gd-bis-5-HT-DTPA was investigated in mice bearing matrix gel implants containing immobilized human MPO and glucose oxidase using ^111^In-labeled bis-5-HT-DTPA (^111^In-bis-5-HT-DTPA) as a surrogate tracer for the MRI agent (6). The synthesis of ^111^In-bis-5-HT-DTPA has been described by Chen et al. (6). The radiochemical yield, purity, and specific activity of the labeled compound were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gd-bis-5-HT-DTPA%20in%20vitro&cmd=DetailsSearch)]

The r_1_ relaxivity value of Gd-bis-5-HT-DTPA was determined to be 5.6 mM−^1^s−^1^ (5). The reduction potential of bis-5-HT-DTPA alone was reported to be 0.63 (5).

The stability of Gd-bis-5-HT-DTPA was studied in a transmetallation reaction as described by Rodriguez et al. (5). Briefly, 2.5 mM Gd-bis-5-HT-DTPA in 1 mL phosphate buffer (pH 7.0) was exposed 10 μL ZnCl_2_ (250 mM) in water, and the T_1_ values of the solution were measured for 3 days at 40°C. Two different parameters were measured: the kinetic index, which is the time required to reach 80% of the initial R_1_ value, and the thermodynamic index, which is the ratio of the R_1_ value after 3 days (4,320 min) and the R_1_ at t = 0 (% of R_1_ after 3 days). The kinetic index and the thermodynamic index of Gd-bis-5-HT-DTPA were determined to be 2,866 min and 0.76, respectively.

In another study, up to 5 mM Gd-bis-5-HT-DTPA was shown to be non-toxic to NIH 3T3 cells for at least 12 h as determined with a cell metabolic activity assay using 3-(4,5-dimethylthiazol-2-yl)2,5-diphenyl-tetrazolium bromide (MTT) (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gd-bis-5-HT-DTPA%20rodentia&cmd=DetailsSearch)]

The biodistribution of Gd-bis-5-HT-DTPA was investigated in mice bearing basement membrane matrix gel implants containing 15 U immobilized human MPO and 4 U glucose oxidase (generates H_2_O_2_ and is necessary to detect the activity of MPO) on the right thigh as described by Chen et al. (6). This model system was used to mimic the accumulation of MPO in the inflamed tissue. For use as a control, the left thigh of each animal was implanted with a matrix gel containing no enzymes. The animals (n = 3 animals/group) were injected intravenously with a saline solution of 2.96–3.70 MBq (80–100 μCi) ^111^In-bis-5-HT-DTPA and subjected to fused single-photon emission computed tomographic and computed tomographic (SPECT/CT) imaging 3 h postinjection (p.i.). At 6 h p.i., the animals were euthanized to determine the percent dose of radioactivity present per gram tissue (% ID/g) of the major organs. From the SPECT/CT images, it was clear that high amounts of radioactivity were present in the gel matrix containing the MPO on the right leg of the animal, but almost no tracer was detected in the control gel matrix on the left leg. A 2.3 ± 0.3-fold increase in radioactivity was observed in the right leg compared to the control leg. The biodistribution data showed that 90% ID was excreted by the animals by 6 h p.i. Little radioactivity was detected in most organs except the spleen, bowel, kidney, and liver, which contained ~2% ID/g, ~1.5% ID/g, ~0.75% ID/g, and ~0.5% ID/g of the label, respectively.

To visualize the accumulation of Gd-containing contrast agents in gel matrices containing MPO, other animals (n = 3 mice/group) were subjected to magnetic resonance imaging (MRI) at 3 h after an injection of Gd-DTPA, Gd-bis-tyramide-DTPA, Gd-5-HT-DOTA, or Gd-bis-5-HT-DTPA (6). Contrast enhancement obtained from the MRI images was reported as relative contrast/noise ratios (CNR) as described by Chen et al. (6). An increased CNR was observed only in the right leg of animals injected with Gd-5-HT-DOTA (CNR = 1.7, P < 0.001) or Gd-bis-5-HT-DTPA (CNR = 1.9, P < 0.001).

Rodriguez et al. showed that MRI with Gd-bis-5-HT-DTPA could detect as little as 0.005 U MPO/mg matrix gel implants in mice, indicating that the agent was suitable for detection of the early stages of inflammation in a murine model (5).

To investigate the induction and secretion of mouse endogenous MPO, matrix gel containing MPO and embedded with Escherichia coli lipopolysaccharide (LPS) was implanted in the right thigh of mice (n = 3 animals) (6). Matrix gel implants in the left thigh of the animals contained no LPS as a control. Four days later, an examination of the implant in the right legs showed the presence of a large number of cells that were positive for MPO by immunostaining; however, the implants in the left legs showed the presence of few cells and were negative for MPO by immunostaining. When Gd-bis-5-HT-DTPA was administered to the animals, there was a 1.3-fold increase in contrast material on the right side for at least 50 min after the Gd-bis-5-HT-DTPA injection (P < 0.001). No such increase was observed in the left thigh of the mice or when the animals were injected with Gd-DTPA (6).

In another study, MRI with Gd-bis-5-HT-DTPA was shown to distinguish inflammation from tumor and peritumoral edema in rats (3).

From these studies, the investigators concluded that MPO activity in matrix implants and rodent inflamed tissue can be detected with MPO-sensitive MRI probes (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gd-bis-5-HT-DTPA%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gd-bis-5-HT-DTPA%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Gd-bis-5-HT-DTPA%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

Some of the studies mentioned in this chapter were supported by National Institutes of Health grants P50-CA86355, R24-CA92782, R01-HL078641, and R01-EB000858; National Cancer Institute grant R21-CA135526; National Institute for Neurological Disorders grants R01-NS070835 and R01-NS072167; and the National Heart, Lung, and Blood Institute grant K08-HL081170.

## References

1 Gleeson M., Bishop N.C., Stensel D.J., Lindley M.R., Mastana S.S., Nimmo M.A. (2011). The anti-inflammatory effects of exercise: mechanisms and implications for the prevention and treatment of disease. Nat Rev Immunol.
2 Maskrey B.H., Megson I.L., Whitfield P.D., Rossi A.G. (2011). Mechanisms of resolution of inflammation: a focus on cardiovascular disease. Arterioscler Thromb Vasc Biol.
3 Kleijn A., Chen J.W., Buhrman J.S., Wojtkiewicz G.R., Iwamoto Y., Lamfers M.L., Stemmer-Rachamimov A.O., Rabkin S.D., Weissleder R., Martuza R.L., Fulci G. (2011). Distinguishing inflammation from tumor and peritumoral edema by myeloperoxidase magnetic resonance imaging. Clin Cancer Res.
4 Mika D., Guruvayoorappan C. (2011). Myeloperoxidase: the yin and yang in tumour progression. J Exp Ther Oncol.
5 Rodriguez E., Nilges M., Weissleder R., Chen J.W. (2010). Activatable magnetic resonance imaging agents for myeloperoxidase sensing: mechanism of activation, stability, and toxicity. J Am Chem Soc.
6 Chen J.W., Querol Sans M., Bogdanov A., Weissleder R. (2006). Imaging of myeloperoxidase in mice by using novel amplifiable paramagnetic substrates. Radiology.